# ^111^In-Diethylenetriamine pentaacetic acid-single-walled nanotubes

Chemical name: | ^111^In-Diethylenetriaminepentaacetic acid-single-walled nanotubes
Abbreviated name: | ^111^In-DTPA-SWNTs
Synonym:
Agent category: | Nanoparticle
Target: | Non-targeted
Target category: | Other
Method of detection: | SPECT, gamma planar
Source of signal\contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SWNT)]

Optical fluorescence imaging is increasingly used to visualize biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Carbon nanotubes are made of fullerene carbon units, which respond to local dielectric changes without photo-bleaching (3, 4). They can be tuned to a range of wavelengths for NIR absorption, thus providing broad excitation profiles and high absorption coefficients. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds for in vitro and in vivo studies (5). Single-walled carbon nanotubes (SWNTs) have a diameter of 1–5 nm and a length of 300–1,000 nm. They have been shown to be nontoxic to cells in vitro (6). However, there have been limited studies of their in vivo toxicological and pharmacological profiles in small animals. SWNTs have been conjugated with diethylenetriamine pentaacetic acid (DTPA) and radiolabeled with ^111^In to form ^111^In-DTPA-SWNTs for quantitative biodistribution studies in small animals (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+synthesis)]

Singh et al. (7) introduced DTPA groups to NH_2_-SWNTs (0.5 mmol NH_2_/g) by incubation of NH_2_-SWNTs (1.4 nm in diameter and 300–1,000 nm in length) with diisopropylethylamine and DTPA dianhydride for 3 h at room temperature. DTPA-SWNTs were diluted with water and lyophilized twice. DTPA-SWNTs were complexed with ^111^In-citrate for 60 min at room temperature. ^111^In-DTPA-SWNTs were used without further purification. ^111^In-DTPA-SWNTs-3 contained 0.5 mmol/g DTPA with one ^111^In ion per ~70,000 DTPA, whereas ^111^In-DTPA-SWNTs-5 contained 0.3 mmol/g DTPA groups with one ^111^In ion per ~42,000 DTPA. The specific activity of both tracers was ~12.3 MBq/mg (~0.33 mCi/mg)

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+in+vitro)]

Yehia et al. (8) performed transmission electron microscopy (TEM) and confocal Raman spectroscopy using human HeLa cells after incubation with SWNTs for up to 60 h at 37°C. SWNTs were taken up by HeLa cells in a time-dependent manner as determined with confocal Raman spectroscopy. TEM revealed that SWNTs were found in intracellular vacuoles but not in the nucleus. SWNTs did not affect the growth rates of HeLa cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+%20rodentia)]

Singh et al. (7) studied short-term biodistribution in normal mice (n = 3 mice/group) up to 24 h after intravenous injection of 60 µg ^111^In-DTPA-SWNTs-3 or ^111^In-DTPA-SWNTs-5 with a total radioactivity of 0.74 MBq (20 µCi). Both nanotubes (-3 versus -5) accumulated quickly in the kidney (10.5 versus 20.7% injected dose (ID)/g), skin (1.9 versus 9.1% ID/g), muscle (6.2 versus 8.6% ID/g), blood (2.7 versus 3.2% ID/g), and lung (0.47 versus 1.35% ID/g) at 30 min after injection. Lower levels were observed in the heart (0.22 versus 0.52% ID/g), liver (0.19 versus 0.20% ID/g), and spleen (0.42 versus 0.23% ID/g). The nanotubes were cleared from all tissues in 3–24 h. ^111^In-DTPA-SWNTs-3 had a half-life of 3.5 h in blood, and ^111^In-DTPA-SWNTs-5 had a half-life of 3.0 h. TEM analysis of urine indicated that the nanotubes were excreted into urine intact.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+human)]

No publication is currently available.

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Hersam M.C. (2008). Progress towards monodisperse single-walled carbon nanotubes. Nat Nanotechnol.
4 Barone P.W., Baik S., Heller D.A., Strano M.S. (2005). Near-infrared optical sensors based on single-walled carbon nanotubes. Nat Mater.
5 Klumpp C., Kostarelos K., Prato M., Bianco A. (2006). Functionalized carbon nanotubes as emerging nanovectors for the delivery of therapeutics. Biochim Biophys Acta.
6 Chin S.F., Baughman R.H., Dalton A.B., Dieckmann G.R., Draper R.K., Mikoryak C., Musselman I.H., Poenitzsch V.Z., Xie H., Pantano P. (2007). Amphiphilic helical peptide enhances the uptake of single-walled carbon nanotubes by living cells. Exp Biol Med (Maywood).
7 Singh R., Pantarotto D., Lacerda L., Pastorin G., Klumpp C., Prato M., Bianco A., Kostarelos K. (2006). Tissue biodistribution and blood clearance rates of intravenously administered carbon nanotube radiotracers. Proc Natl Acad Sci U S A.
8 Yehia H.N., Draper R.K., Mikoryak C., Walker E.K., Bajaj P., Musselman I.H., Daigrepont M.C., Dieckmann G.R., Pantano P. (2007). Single-walled carbon nanotube interactions with HeLa cells. J Nanobiotechnology.